# Alexa Fluor 488–conjugated anti-carcinoembryonic antigen monoclonal antibody

Chemical name: | Alexa Fluor 488–conjugated anti-carcinoembryonic antigen monoclonal antibody
Abbreviated name: | AlexaFluor 488 anti-CEA MAb
Synonym:
Agent Category: | Monoclonal antibody
Target: | Carcinoembryonic antigen (CEA)
Target Category: | Antibody-ligand binding
Method of detection: | Fluorescence imaging
Source of Signal/Contrast: | Alexa Fluor 488
Activation: | No
Studies: | - In vitro; - Rodents | Click here for protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=38522495) and nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=databasead&logdbfrom=protein) information regarding human CEA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Carcinoembryonic+antigen)]

Surgical resection is the most common treatment for colorectal and pancreatic cancers (1, 2). Therefore it is important to be able to detect the primary and metastatic lesions of these cancers for proper surgical resection and treatment. Although patients with colorectal cancers have more than one surgical option for treatment, the aggressive nature, and the usually late-stage detection, of pancreatic cancer often results in a negative outcome for patients (3). Also, chemotherapeutic treatments have a marginal effect on the survival of pancreatic cancer patients, which suggests that complete resection of the primary and metastatic lesions could possibly improve the chances of a positive treatment outcome (2, 4, 5). The carcinoembryonic antigen (CEA) has been shown to be a marker for several cancers originating from the endodermally derived epithelium of the digestive tract, including tissue from the embryonic gut, pancreas, and liver (6, 7). Because CEA is usually expressed at high levels in adenocarcinomas of the colon and the pancreatic ducts, it is used as a serum marker for the detection of these cancers and to monitor patient response after treatment (8, 9). Kaushal et al. evaluated the use of a fluorophore-labeled anti-CEA monoclonal antibody (MAb) to detect colon and pancreatic cancer in nude mice bearing human xenograft tumors (10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=fluorophore+conjugated+anti+CEA+antibody+synthesis)]

The anti-CEA MAb was purchased from commercial sources and conjugated with Alexa Fluor 488 dye according to the manufacturer’s instructions (10). For the conjugation, the MAb was reconstituted in sodium bicarbonate and mixed with the dye as recommended by the manufacturer. The MAb-dye mixture was incubated for 1 h at room temperature and then overnight at 4°C. Unconjugated dye was removed with centrifugation on a column (type of column was not specified). A similar procedure was also used to conjugate the anti-CEA MAb with Oregon Green. A control IgG antibody was similarly labeled with the fluorophores. The fluorophore:MAb ratio of the labeled antibodies was reported to be 3–4:1 (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor+488+anti-CEA+antibody+in+vitro)]

Kaushal et al. investigated the expression of CEA with Alexa Fluor 488 anti-CEA MAb in several human cell lines of pancreatic or colon cancer origin (see Kaushal et al. for a list of all the cell lines (10)). Positive staining was indicated by fluorescence staining above background observed with the Alexa Fluor–conjugated IgG. Seven of the 10 pancreatic cell lines (70%) showed an expression of CEA. Among the colon cell lines, four of the six pancreatic cell lines (67%) were positive for the expression of CEA. A primary human colon cancer tissue, Colo4104, was also reported to express CEA. No blocking studies with the unconjugated anti-CEA MAb were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor+488+anti-CEA+antibody+rodentia)]

The fluorophore used for the in vivo studies was selected on the basis of comparing fluorescence imaging with the anti-CEA MAb conjugated to either the Oregon Green or the Alexa Fluor 488 dye (10). Animals (n = 3 per fluorophore dose) bearing human pancreatic cancer cell ASPC-1 xenograft tumors were treated with various doses of either fluorophore-conjugated MAb and imaged 24 h later. The Alexa Fluor–conjugated MAb was reported to show the highest fluorescence intensity at the three lower doses with a marginal increase at the higher doses. The Oregon Green conjugated MAb had a lower fluorescence intensity compared to the Alexa Fluor–conjugated MAb at all doses.

Kaushal et al. investigated the expression of CEA in an in vivo athymic mouse model (10). The mice (n = 3 animals per cell line) were respectively implanted (subcutaneously) with human ASPC-1, BxPC-3, CFPAC, Panc-1 and Capan-1 pancreatic cancer, LS174T colon cancer, and the primary Colo4104 cancer cell lines. The tumors were allowed to grow for 7–14 days; when the tumors were 1–2 mm in diameter, the animals were injected with the Alexa Fluor 488 anti-CEA MAb through the tail vein. All the tumors, including those from the primary colon cancer cell line, were reported to be positive for CEA. No competition binding studies were reported. A time course for the imaging of pancreatic tumors was also studied. Animals bearing human pancreatic cell tumors were injected with the fluorophore-conjugated MAb and imaged at various time periods from 30 min to 15 days (n = 2 animals per time point) after treatment with the conjugated MAb. The fluorescence signal was reported to steadily increase for up to 24 h after the conjugated-CEA MAb treatment, but it was observed to be minimal after 15 days.

CEA expression was also investigated in orthotopic tumors implanted in nude mice (n = 3 animals per cell line) (10). Tumors were established with direct injection of BxPC-3 cells into the pancreas. Similarly, colorectal tumors were established in the animals with direct injection of the Colo4104 cells. The tumors were allowed to grow as described above, and the animals were treated with the conjugated-CEA MAb as described above. None of the tumors were easily visualized with standard bright light illumination, but with fluorescence imaging the lesions were very clear and the extent of invasion was observed to be much larger than apparent with standard illumination. The investigators reported that no fluorescence was observed when the animals were injected with the conjugated-IgG (control).

Alexa Fluor 488 anti-CEA MAb was also evaluated for the visualization of intra-abdominal metastases of pancreatic and colon cancers (n = 3 animals per cell line) by implanting ASPC-1 (human pancreatic cancer origin) and Colo4104 (human colorectal cancer origin) cells into the peritoneal cavity of nude mice (10). The implants were allowed to grow for 1–2 weeks, and then the animals were injected with the conjugated-CEA MAb through the tail vein. Control animals received a fluorophore-conjugated IgG treatment. The animals were then imaged 24 h later with bright field and fluorescence illumination. Small peritoneal implants were reported to be visualized in the bowel and mesentery only with the conjugated-CEA MAb. No blocking studies with the unconjugated anti-CEA MAb were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor+488+anti+CEA+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=AlexaFluor+488+anti+CEA+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

This study was supported in part by a National Institutes of Health grant (CA109949-03).

## References

1 Figueredo A., Coombes M.E., Mukherjee S. (2008). Adjuvant Therapy for completely resected Stage II Colon Cancer. Cochrane Database Syst Rev.
2 Wagner M., Redaelli C., Lietz M., Seiler C.A., Friess H., Buchler M.W. (2004). Curative resection is the single most important factor determining outcome in patients with pancreatic adenocarcinoma. Br J Surg.
3 Wray C.J., Ahmad S.A., Matthews J.B., Lowy A.M. (2005). Surgery for pancreatic cancer: recent controversies and current practice. Gastroenterology.
4 Boeck S., Ankerst D.P., Heinemann V. (2007). The role of adjuvant chemotherapy for patients with resected pancreatic cancer: systematic review of randomized controlled trials and meta-analysis. Oncology.
5 Bria E., Milella M., Gelibter A., Cuppone F., Pino M.S., Ruggeri E.M., Carlini P., Nistico C., Terzoli E., Cognetti F., Giannarelli D. (2007). Gemcitabine-based combinations for inoperable pancreatic cancer: have we made real progress? A meta-analysis of 20 phase 3 trials. Cancer.
6 Gold P., Freedman S.O. (1965). Specific carcinoembryonic antigens of the human digestive system. J Exp Med.
7 Gold P. Shuster J. Freedman S.O. Carcinoembryonic antigen (CEA) in clinical medicine: historical perspectives, pitfalls and projections Cancer 1978 42Suppl3 1399 405 361199
8 Locker G.Y., Hamilton S., Harris J., Jessup J.M., Kemeny N., Macdonald J.S., Somerfield M.R., Hayes D.F., Bast R.C. (2006). ASCO 2006 update of recommendations for the use of tumor markers in gastrointestinal cancer. J Clin Oncol.
9 Goldstein M.J., Mitchell E.P. (2005). Carcinoembryonic antigen in the staging and follow-up of patients with colorectal cancer. Cancer Invest.
10. Kaushal, S., M.K. McElroy, G.A. Luiken, M.A. Talamini, A.R. Moossa, R.M. Hoffman, and M. Bouvet, Fluorophore-conjugated anti-CEA Antibody for the Intraoperative Imaging of Pancreatic and Colorectal Cancer. J Gastrointest Surg, 2008.